# Gadolinium-1,4,7,10-tetraazacyclododecane-N',N'',N''',N''''-tetraacetic acid-Gly-Pro-D-Leu-D-Ala-NHOH

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-N',N'',N''',N''''-tetraacetic acid-Gly-Pro-D-Leu-D-Ala-NHOH
Abbreviated name: | P947
Synonym: | Gd-DOTA-FN-439
Agent category: | Peptide
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=13177712), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=75709180) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4316&ordinalpos=2&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about MMP.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P947)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play an important role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degradation of the basement membrane and ECM (3). Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (4-7).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (8, 9). Gd-Labeled diethylenetriaminepentaacetic acid (Gd-DTPA) was the first intravenous magnetic resonance imaging (MRI) contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Various macromolecular Gd complexes have demonstrated superior contrast enhancement for MRI of the vasculature and carcinomas (10-12); however, these Gd complexes cannot proceed into further clinical development because of high tissue accumulation and slow excretion of toxic Gd ions. Furthermore, they are largely nonspecific. Gly-Pro-D-Leu-D-Ala-NHOH was found to be a broad-spectrum inhibitor of MMP-1, -2, -3, -8, -9, and -13 (13). Gd-1,4,7,10-tetraazacyclododecane-N',N'',N''',N''''-tetraacetic acid (DOTA)-Gly-Pro-D-Leu-D-Ala-NHOH (P947) has been developed to detect MMP activities in atherosclerotic plaques.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P947+synthesis)]

P947 was prepared by coupling Gly-Pro-D-Leu-D-Ala-NHOH to DOTA (13). P947 is a Gd(III) complex of a bi-functional DOTA chelate conjugated via a phenylbutyric linker with a thiourea function to the tetrapeptidyl hydroxamic acid Gly-Pro-D-Leu-D-Ala-NHOH. It has a molecular weight of 1,210 Da and the r1 relaxivity value of 5.5 mM^-1^ s^-1^ in water at 1.5 T and 37°C, whereas Gd-DOTA has the r1 relaxivity value of 3.7 mM^-1^ s^-1^.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P947+in+vitro)]

P947 exhibited 50% inhibition concentration (IC_50_) values of 100 µM for MMP-14, 10 µM for MMP-3 and MMP-9, 1 µM for MMP-1, MMP-2, and MMP-13, and 0.1 µM for MMP-8 (13). Immunohistochemical measurements of human and rabbit atherosclerotic aortas revealed the presence of various MMPs in the aortas with higher P947 accumulation than Gd-DOTA. Gly-Pro-D-Leu-D-Ala-NHOH blocked P947 accumulation in the rabbit experiments.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P947+rodentia)]

Lancelot et al. (13) used a 9.4-T MRI scanner to perform in vivo MRI in apolipoprotein E–deficient (ApoE^-/-^) mice (n = 8). Injection of P947 (0.1 mmol/kg) provided strong MRI contrast enhancement in the atherosclerotic aortic wall within 1 h of injection; this enhancement was still visualized up to 22 h. The contrast enhancement was 95%, 50%, 20%, and 10% at 1, 2, 3, and 22 h after injection, respectively. On the other hand, Gd-DOTA provided only a diffuse contrast, and the atherosclerotic aortic wall was not clearly outlined with little contrast enhancement. No enhancement was observed in the aortic wall of the wild-type mice after injection of P947. Ex vivo biodistribution studies in ApoE^-/-^ mice showed that the organ with the highest uptake was the kidney (90 nmol Gd/g), followed by the liver (18 nmol Gd/g), at 30 min after injection of P947. The liver uptake of P947 was three-fold higher than that of Gd-DOTA, whereas no differences were observed in the kidney, muscle, and plasma. The plasma half-life was 30 min for P947 and 15 min for Gd-DOTA. P947 levels in the atherosclerotic arteries were 3-fold higher than Gd-DOTA levels. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P947+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P947+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P947+human)]

No publication is currently available.

## NIH Support

HL78667, R01 HL71021

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
9 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
10 Schmiedl U., Ogan M., Paajanen H., Marotti M., Crooks L.E., Brito A.C., Brasch R.C. (1987). Albumin labeled with Gd-DTPA as an intravascular, blood pool-enhancing agent for MR imaging: biodistribution and imaging studies. Radiology.
11 Gossmann A., Okuhata Y., Shames D.M., Helbich T.H., Roberts T.P., Wendland M.F., Huber S., Brasch R.C. (1999). Prostate cancer tumor grade differentiation with dynamic contrast-enhanced MR imaging in the rat: comparison of macromolecular and small-molecular contrast media--preliminary experience. Radiology.
12 Preda A., van Vliet M., Krestin G.P., Brasch R.C., van Dijke C.F. (2006). Magnetic resonance macromolecular agents for monitoring tumor microvessels and angiogenesis inhibition. Invest Radiol.
13 Lancelot E., Amirbekian V., Brigger I., Raynaud J.S., Ballet S., David C., Rousseaux O., Le Greneur S., Port M., Lijnen H.R., Bruneval P., Michel J.B., Ouimet T., Roques B., Amirbekian S., Hyafil F., Vucic E., Aguinaldo J.G., Corot C., Fayad Z.A. (2008). Evaluation of matrix metalloproteinases in atherosclerosis using a novel noninvasive imaging approach. Arterioscler Thromb Vasc Biol.